# ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-1,2-diaminoethane-γ-5,8-dideazfolic acid (P3238)

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-1,2-diaminoethane-γ-5,8-dideazfolic acid (P3238)
Abbreviated name: | ^68^Ga-P3238
Synonym: | ^68^Ga-NODAGA-5,8-dideazfolic acid
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3238)]

Folic acid (folate) is a water-soluble B vitamin (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher-affinity receptor (dissociation constant (K_d_) = 0.5 nM) that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells have been found to overexpress folate receptors (2). More than 90% of human ovarian and endometrial cancers express the high-affinity folate receptor, which is absent in the corresponding normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the high-affinity folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have also been found to have the high-affinity folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate, ^99m^Tc-EC-folate, and [^18^F]FBA-folate) have been studied in tumor imaging (4-8). Deferoxamine (DF), a chelating agent, was conjugated to folic acid to form a mixture of two isomers, DF-α-folate and DF-γ-folate. Only the DF-γ-folate isomer was able to displace [^3^H]folic acid from its receptors, with a 50% inhibition concentration similar to that of folic acid (2.5 nM versus 2.4 nM) (9). Fani et al. (10) prepared a γ-folate conjugate with tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) and 1,2-diaminoethane as a spacer to form P3026 (http://www.ncbi.nlm.nih.gov/books/NBK55064/), which was labeled with ^68^Ga for positron emission tomography (PET) imaging of folate receptors in tumors. To further the quest for a ^68^Ga-folate conjugate for clinical application, 5,8-dideazfolic acid was conjugated to 1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid (NODAGA) via 1,2-diaminoethane as a linker between the NODAGA and 5,8-dideazfolic acid (P3238) (11). ^68^Ga-P3238 was evaluated as a PET agent for imaging folate receptor expression in a mouse tumor model. ^68^Ga-P3238 exhibited a lower tumor/blood ratio than ^68^Ga-P3246 (^68^Ga-NODAGA-folate) but a higher ratio than ^68^Ga-3026 in the same tumor model.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20synthesis)]

Fani et al. (11) coupled P3238 (12 nmol) with ^68^Ga in sodium acetate buffer (pH 4.0) for 10 min at 25°C to yield ^68^Ga-P3238 with >92% radiochemical purity. Radiochemical yields exceeded 95% with a specific activity of 30 MBq/nmol (0.81 mCi/nmol). ^67^Ga-P3238 was similarly radiolabeled with a specific activity of ~3 MBq/nmol (0.081 mCi/nmol). ^68^Ga-P3246 was prepared with similar specific activity as ^68^Ga-P3238.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB cell line folate receptors were studied with ^67^Ga-P3238 saturation binding studies at 4°C (11). ^67^Ga-P3238 showed a K_d_ (affinity constant) of 7.21 ± 2.46 nM, which was slightly higher than the K_d_ value (5.61 ± 0.96 nM) for ^67^Ga-P3246. ^67/68^Ga-P3238 (2.5 nM) was rapidly associated (bound to the cell surface and internalized) with KB cells at 37°C, with 50% of incubation dose (ID) at 30 min and 60% ID at 4 h. Approximately 10% ID ^67/68^Ga-P3238 was internalized at 4 h. Excess folate blocked the cell-associated radioactivity to <1% ID. Approximately 71% of radioactivity was retained in the cells after 4 h incubation in fresh medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20rodentia)]

Fani et al. (11) performed ex vivo biodistribution studies of 0.4 nmol ^67/68^Ga-P3238 in nude mice (n = 3–5/group) bearing KB tumor xenografts. Accumulation of ^67/68^Ga-P3238 in the KB tumors was 10.95 ± 2.12, 12.89 ± 1.41, and 14.88 ± 2.28% injected dose/gram (ID/g) at 1, 2, and 4 h after injection, respectively. The organ with the highest accumulation at 4 h after injection was the kidneys (112% ID/g), followed by the salivary gland (10.91% ID/g), adrenal (3.8% ID/g), pancreas (2.8% ID/g), liver (2.5% ID/g), heart (2.1% ID/g), muscle (1.7% ID/g), and stomach (1.7% ID/g). The accumulation in the blood was low (0.1% ID/g) at 4 h. The tumor/blood ratios were 57, 99, 254, and 151 at 1, 2, 4, and 24 h, respectively. Pretreatment with excess folate (40 nmol, 5 min before ^67^Ga-P3238 injection) reduced the radioactivity accumulation by >84% in the folate receptor-positive tumor, salivary glands, and kidneys at 4 h after injection. Pretreatment with pemetrexed (60 min before ^67/68^Ga-P3238 injection), a folate analog metabolic inhibitor, significantly reduced the kidney accumulation of ^67^Ga-P3238 by >70% at 1 h after injection (P < 0.05). On the other hand, little inhibition by pemetrexed was observed in the tumor and other organs. ^67/68^Ga-P3238 exhibited lower tumor/blood ratios than ^67/68^Ga-P3246 (tumor/blood ratios of 81 at 1 h, 207 at 2 h, and 254 at 4 h). No PET imaging study was performed with ^68^Ga-P3238.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P3246%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.
9 Wang S., Lee R.J., Mathias C.J., Green M.A., Low P.S. (1996). Synthesis, purification, and tumor cell uptake of 67Ga-deferoxamine--folate, a potential radiopharmaceutical for tumor imaging. Bioconjug Chem.
10 Fani M., Wang X., Nicolas G., Medina C., Raynal I., Port M., Maecke H.R. (2011). Development of new folate-based PET radiotracers: preclinical evaluation of Ga-DOTA-folate conjugates. Eur J Nucl Med Mol Imaging.
11 Fani M., Tamma M.L., Nicolas G.P., Lasri E., Medina C., Raynal I., Port M., Weber W.A., Maecke H.R. (2012). In Vivo Imaging of Folate Receptor Positive Tumor Xenografts Using Novel (68)Ga-NODAGA-Folate Conjugates. Mol Pharm.